# ^213^Bi/^211^At-Labeled MX35, an anti–sodium-dependent phosphate transport protein 2b (NaPi2b) murine monoclonal antibody

Chemical name: | ^213^Bi/^211^At-Labeled MX35, an anti–sodium-dependent phosphate transport protein 2b (NaPi2b) murine monoclonal antibody
Abbreviated name: | [^213^Bi]MX35 and [^211^At]MX35
Synonym:
Agent Category: | Antibody
Target: | Sodium-dependent phosphate transport protein 2b (NaPi2b)
Target Category: | Transporter
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^213^Bi and ^211^At
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MX35&cmd=DetailsSearch)]

The sodium-dependent phosphate transporter NaPi2b is overexpressed in 70%–90% of ovarian cancers (1). Although NaPi2b is believed to maintain phosphate homeostasis in the human body, the exact role of this transporter in neoplastic transformation and ovarian cancer tumor growth is unclear. Investigators have developed a murine anti- NaPi2b monoclonal antibody (mAb), designated MX35, and showed that ^211^At-labeled MX35 ([^211^At]MX35) can be used for the intraperitoneal radioimmunotherapy (RIT) of micrometastatic growth of OVCAR-3 cells (http://www.atcc.org/attachments/17430.pdf) (human ovarian cancer cells) in the peritoneum of nude mice (2). In a phase 1 study, the pharmacokinetics and dosimetry of the ^211^At-labeled MX35 F(ab')_2_ fragment were investigated in patients with ovarian cancer (3). From this study it was apparent that ^211^At (half-life, 7.2 h) is likely to irradiate other normal organs in the body by travelling through blood circulation (3, 4). In addition, it was reported that the efficacy of ^211^At reduces with the increase in lesion size because the radionuclide has a path length of 46–68 μm in the tissue (1, 3). In this regard, ^213^Bi appears to be a more suitable radionuclide for RIT of the ovarian cancer lesions because it has a short half-life (~46 min), a path length of 82 μm in the tissue, and probably does not travel to other organs because of its short half-life (3). As an extension of the earlier studies, the investigators labeled MX35 with ^213^Bi ([^213^Bi]MX35) and compared its biodistribution with that of [^211^At]MX35 in normal nude mice (3). It is pertinent to mention that ^213^Bi is transformed primarily to ^213^Po (half-life, 4.2 sec) which in turn decays to ^209^Pb (half-life, 3.2 h). There is a probability that the two nuclear transformations of ^213^Bi would occur during circulation and the final radionuclide (^209^Pb) may not be retained on the chelating agent-mAb complex. Therefore, the biodistribution of the labeled mAb presented here may not be that of the mAb itself.

### Related Resource Links

Ovarian cancer related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Ovarian+cancer+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human NaPi2b (MX35 antigen) protein (http://www.ncbi.nlm.nih.gov/nuccore/NM_006424.2) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_006424.2) sequences

Clinical trials (http://clinicaltrials.gov/ct2/results?term=ovarian+cancer) on ovarian cancer

Click here (http://ie.lbl.gov/education/isotopes.htm) for information regarding radionuclide half-lives and other related information.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=213Bi-MX35%20synthesis&cmd=DetailsSearchhttp://www.ncbi.nlm.nih.gov/pubmed?term=213Bi-MX35%20synthesis&cmd=DetailsSearch)]

The MX35 used for studies reported in this chapter was obtained from a cancer research institute in Europe (3). The mAb was conjugated with 2-(p-SCN-benzyl)-cyclohexyl-A-diethylenetriamine pentaacetic acid (CHX-A''-DTPA), a metal chelator, before it was labeled with ^213^Bi ([^213^Bi]MX35). On average, two CHX-A''-DTPA molecules were available on each molecule of MX35 as determined with a spectroscopic method. The radiochemical yield (RCY) of the labeling reaction was 20%–51%, and the radiochemical purity (RCP) of the final radiolabeled product was 90%–97%. One atom of ^213^Bi was reported to be attached in every 1,500 molecules of MX35 (3).

To label MX35 with ^211^At, the mAb was first conjugated with N-succinimidyl-3-(trimethylstannyl)benzoate (m-MeATE) as described by Elgqvist et al. (2). The RCY and RCP of [^211^At]MX35 were 25%–40% and >95%, respectively, and the labeled mAb had a specific activity of 134 ± 25 kBq/6.6 pmol (3.62 ± 0.675 μCi/6.6 pmol) (2). The RCY of [^211^At]MX35 used in studies reported in this chapter was 60%–63%, with a RCP of 96% (3). There was one atom of ^211^At in every 500 molecules of MX25 (3). The specific activity of the labeled mAb at the end of synthesis was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21958859%5Buid%5D&cmd=DetailsSearch)]

Using OVCAR-3 cells in an in vitro assay, the immunoreactivities of [^213^Bi]MX35 and [^211^At]MX35 were reported to be 58%–70% and 85%–87%, respectively (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=211At-MX35%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^211^At]MX35 was investigated in BALB/c nu/nu nude mice by Elgqvist et al. (5). The mice (n = 5 animals/time point) were injected in the peritoneum with ~1 MBq (27 μCi) of the labeled mAb and euthanized at 3, 6, and 18 h post injection (p.i.). The blood, bone marrow, and organs of interest were harvested from the rodents to determine the amount of radioactivity accumulated in the different tissues, and the organ/blood (O/B) ratios were calculated (Table 1). Little change was observed in the O/B ratios for all the organs during the entire duration of the study (from 3 h to 18 h p.i.).

Table 1: Organ/blood ratios in nude mice with [ ^ 211 ^ At]MX35.

Organ | Time after intraperitoneal injection (hours)
Organ | 3 | 6 | 18
Bone | 0.18 ± 0.04 | 0.29 ± 0.05 | 0.22 ± 0.05
Bone marrow | 0.54 ± 0.12 | 0.60 ± 0.10 | 0.59 ± 0.12
Heart | 0.26 ± 0.05 | 0.36 ± 0.07 | 0.34 ± 0.07
Kidney | 0.27 ± 0.05 | 0.29 ± 0.05 | 0.31 ± 0.05
Liver | 0.30 ± 0.05 | 0.34 ± 0.05 | 0.33 ± 0.07
Lung | 0.48 ± 0.07 | 0.57 ± 0.09 | 0.49 ± 0.09
Spleen | 0.33 ± 0.07 | 0.47 ± 0.09 | 0.48 ± 0.09

For complete data, see Elgqvist et al. ( 5 ).

In another study, the biodistribution of a mixture of [^213^Bi]MX35 and [^211^At]MX35 was studied in BALB/c nu/nu nude mice as described by Gustafsson et al. (3). The animals (n = 4 mice/time point/radiolabeled mAb) were given an intraperitoneal injection of a mixture of [^213^Bi]MX35 and [^211^At]MX35 (2.8–3.1 MBq (75.6–83.7 μCi) and 0.14–0.16 MBq (3.78–4.32 μCi), respectively), and the mice were euthanized at 15, 45, 90, and 180 min p.i. The amount of radioactivity accumulated in the organs of interest was measured and presented as percent of injected dose per gram tissue (% ID/g). An analysis of the data showed that the radioactivity measured after an injection of [^213^Bi]MX35 and [^211^At]MX35 had a similar pattern of biodistribution in the various organs of the nude mice. Low levels of radioactivity were observed in all the tissues with both the radiolabeled mAbs. However, a slightly higher amount of ^211^At was detected in the throat (taken to represent the thyroid; see below for explanation) at 90 min p.i. (~2.5% ID/g) and 180 min p.i. (~6% ID/g) compared with the amount of ^213^Bi (~2.0% ID/g and ~5% ID/g at 90 min p.i. and 180 min p.i., respectively). A higher amount of ^213^Bi was present in the kidneys (~5% ID/g and ~7.5% ID/g at 90 min p.i. and 180 min p.i., respectively) compared with the amount of ^211^At/^209^Pb (~2.5% ID/g and ~5% ID/g at 90 min p.i. and 180 min p.i., respectively). The investigators mentioned that these observations were not unexpected because it is known that ^211^At accumulates in the thyroid and that free ^213^Bi tends to accumulate in the kidneys (3). No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=211At-MX35%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=211At-MX35%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=211At-MX35%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Gryshkova V., Lituiev D., Savinska L., Ovcharenko G., Gout I., Filonenko V., Kiyamova R. (2011). Generation of monoclonal antibodies against tumor-associated antigen MX35/sodium-dependent phosphate transporter NaPi2b. Hybridoma (Larchmt).
2 Elgqvist J., Andersson H., Back T., Hultborn R., Jensen H., Karlsson B., Lindegren S., Palm S., Warnhammar E., Jacobsson L. (2005). Therapeutic efficacy and tumor dose estimations in radioimmunotherapy of intraperitoneally growing OVCAR-3 cells in nude mice with (211)At-labeled monoclonal antibody MX35. J Nucl Med.
3 Gustafsson A.M., Back T., Elgqvist J., Jacobsson L., Hultborn R., Albertsson P., Morgenstern A., Bruchertseifer F., Jensen H., Lindegren S. (2012). Comparison of therapeutic efficacy and biodistribution of 213Bi- and 211At-labeled monoclonal antibody MX35 in an ovarian cancer model. Nucl Med Biol.
4 Elgqvist J., Andersson H., Back T., Claesson I., Hultborn R., Jensen H., Johansson B.R., Lindegren S., Olsson M., Palm S., Warnhammar E., Jacobsson L. (2006). Alpha-radioimmunotherapy of intraperitoneally growing OVCAR-3 tumors of variable dimensions: Outcome related to measured tumor size and mean absorbed dose. J Nucl Med.
5 Elgqvist J., Bernhardt P., Hultborn R., Jensen H., Karlsson B., Lindegren S., Warnhammar E., Jacobsson L. (2005). Myelotoxicity and RBE of 211At-conjugated monoclonal antibodies compared with 99mTc-conjugated monoclonal antibodies and 60Co irradiation in nude mice. J Nucl Med.